# ^64^Cu-Labeled, 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-chelated, and cysteine-modified anti-activated leukocyte cell adhesion molecule diabody

Chemical name: | ^64^Cu-Labeled, 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-chelated, and cysteine-modified anti-activated leukocyte cell adhesion molecule diabody
Abbreviated name: | ^64^Cu-DOTA-CysDb
Synonym:
Agent Category: | Antibodies (diabody)
Target: | Activated leukocyte cell adhesion molecule (ALCAM/CD166)
Target Category: | Adhesion molecules
Method of detection: | Positron emission tomography
Source of signal / contrast: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | No structure available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ALCAM%20and%20imaging)]

The ^64^Cu-labeled, 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (DOTA)-chelated, and cysteine-modified anti-activated leukocyte cell adhesion molecule (ALCAM) diabody (CysDb), abbreviated as ^64^Cu-DOTA-CysDb, was synthesized by McCabe et al. for use with positron emission tomography (PET) of tumors expressing ALCAM (1).

Antibodies have long been considered to be the most attractive agents for molecular imaging because of their high specificity and binding affinity (2, 3). However, the usefulness of full antibodies as imaging agents is limited by their long circulation time in blood (several days to weeks), which requires a long time to optimally accumulate in tumors (1–2 days) (2). Because of their large molecular size (150 kDa), antibodies also exhibit poor tumor-penetrating ability, which leads to poor signal/noise ratio. To improve antibody pharmacokinetics without compromising the affinity and specificity, a promising solution is to reduce the antibody size or alter the Fc receptor-binding domain with protein engineering (2, 3). Indeed, various antibody fragments have been generated, such as single-chain variable fragment (scFv; 25–30 kDa), Fab (~50 kDa) and F(ab')_2_ (~110 kDa) fragments, bivalent scFv (tandem scFv and diabody, 50–60 kDa), and scFv-fusion proteins (80 kDa for minibody and 105 kDa for scFv-Fc) (2, 4). These fragments exhibit good tumor penetration, fast clearance kinetics, high affinity, and high tumor/blood ratio, which are desirable for imaging agents. However, several issues with the use of antibody fragments as imaging agents remain to be solved, one of which is the diverse effects of labeling chemistry on the binding affinity of antibody fragments (5, 6).

To reduce the diverse effects of labeling chemistry, various strategies have been designed. For example, Vaidyanathan and Zalutsky prepared ^18^F-labeled antibody fragments using N-succinimidyl-4-[^18^F]fluorobenzoate ([^18^F]SFB), which reacts with the ε-amino group of surface-exposed lysine residues on proteins (7). Labeling with this approach showed no loss of the antibody fragment affinity. Olafsen et al. further improved efficiency and speed of [^18^F]SFB production by adapting the synthesis to a three-step, one-pot, microwave-assisted method, followed by purification using either a single cartridge or high-performance liquid chromatography (HPLC) (7, 8). Alternatively, McCabe et al. first conjugated the diabody to DOTA, followed by ^64^Cu-radiolabeling through DOTA (1). All these strategies have been reported to be efficient and have fewer diverse effects on the binding affinity of antibody fragments. This chapter summarizes the data obtained with ^64^Cu-DOTA-CysDb. In another chapter, the data obtained with [^18^F]FB-Cys-Db are summarized.

### Related Resource Links:

Nucleotide (http://www.ncbi.nlm.nih.gov/nuccore?term=ALCAM%20and%20homo%20sapiens) and protein (http://www.ncbi.nlm.nih.gov/protein?term=ALCAM%20and%20homo%20sapiens) sequences of ALCAM

Bioassay data for ALCAM (http://www.ncbi.nlm.nih.gov/pcassay?term=ALCAM%20and%20homo%20sapiens) in PubChem

Probes for ALCAM gene (http://www.ncbi.nlm.nih.gov/probe?term=ALCAM%20and%20homo%20sapiens)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21630083)]

The anti-ALCAM CysDb construct was developed via polymerase chain reaction (PCR) amplification of the V_H_ and V_L_ sequences of the anti-ALCAM antibody, followed by cloning of the PCR fragments into the mammalian expression vector pEE12 with insertion of a GlySer-rich, eight amino acid linker between the two single-chain variable fragments (scFv) and with attachment of a cysteine and hexahistidine tag at the C-terminus (1). The expression vector was then transfected into NSo mouse myeloma cells for production of the CysDb. The anti-ALCAM CysDb was purified from NSo terminal cultures with a yield of ~10 mg/L supernatant. SDS-PAGE analysis showed that, under non-reducing conditions, the anti-ALCAM CysDb migration was consistent with its predicted dimeric molecular weight of ~50 kDa, and under reducing conditions the migration was consistent with its predicted monomeric molecular weight. The lack of additional bands on the SDS-PAGE gel and the single peak on the chromatogram indicated high purity of the final products. Size-exclusion chromatography confirmed production of the scFv dimer.

For radiolabeling, the anti-ALCAM CysDb was first conjugated with DOTA by incubating the diabody with DOTA at a molar ratio of 1:200 for 12–16 h at 4°C (1). Size-exclusion chromatography showed that the DOTA-conjugated CysDb (DOTA-CysDb) eluted slightly earlier (22.4 min) than the unconjugated CysDb (23.8 min), and the large peak area corresponding to the conjugate indicated high conjugation efficiency (the ratio of DOTA to CysDb in the final product was not reported). ^64^Cu-Labeling was achieved by incubating 14.8–18.5 MBq (0.4–0.5 mCi) ^64^Cu with 200–300 μg DOTA-CysDb for 50 min at 43°C. The ^64^Cu-labeling efficiency was 82 ± 11% (n = 4). The radiochemical purity and specific activity of ^64^Cu-DOTA-CysDb were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21630083)]

McCabe et al. analyzed the ALCAM expression in two human pancreatic adenocarcinoma cell lines HPAF-II and BxPC-3, and one rat glioma cell line C6 using the mouse anti-human ALCAM monoclonal antibody and flow cytometry (1). The results showed that HPAF-II and BxPC-3 were positive for cell surface ALCAM, while C6 was negative. The specific antibody-binding capacity (ABC) for HPAF-II and BxPC-3 cells was between 2.5 × 10^5^ and 3.0 × 10^5^, respectively (n = 2, detailed data not shown). ABC is a term that provides quantitative information about the number of antibodies binding to the surface molecules on individual cells.

The specific binding of CysDb with ALCAM-positive HPAF-II and BxPC-3 cells was also analyzed with flow cytometry. The affinity, expressed as the equilibrium binding constant, was determined to be in the range of 1–3 nM. The nonspecific binding was minimal. Under fluorescent microscopy and with flow cytometry, the Alexa Fluor 647–labeled CysDb retained the immunoreactivity of the native CysDb and bound specifically to ALCAM-positive cells. The binding affinity of ^64^Cu-DOTA-CysDb was not reported.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21630083)]

MicroPET was performed at 4 h and 21 h, respectively, after tail vein injection of 3.7–6.1 MBq (100–165 μCi, 85–95 Ci/mmol) ^64^Cu-DOTA-CysDb in each nude mouse that had an ALCAM-positive (HPAF-II or BxPC-3) and an ALCAM-negative (C6) subcutaneous tumor (n = 4–5 mice/group) (1). The ALCAM-positive but not the ALCAM-negative tumors were clearly detected at 4 h after injection. Very high signal was observed in the kidneys and liver. Ex vivo gamma counting of tumors and organs harvested at 21 h after injection confirmed specific targeting of the probe, with positive tumor uptakes of 1.8 ± 0.5% and 2.5 ± 0.5% injected dose per gram tissue (ID/g) for HPAF-II and BxPC-3, respectively (P = 0.08). The C6-negative tumor uptake (1.0 ± 0.1% ID/g) was comparable to that seen in the blood (0.7 ± 0.1% ID/g for HPAF-II tumor-bearing mice (P < 0.01) and 0.9 ± 0.1% ID/g for BxPC-3 tumor-bearing mice (P > 0.1)) (Table 1). Uptake differences between ALCAM-positive and ALCAM-negative tumors were statistically significant (P < 0.01 for both HPAF-II versus C6 and BxPC-3 versus C6). The positive/negative tumor uptake ratios were 1.9 ± 0.6 and 2.4± 0.6 for HPAF-II/C6 and BxPC-3/C6, respectively. The positive tumor/blood radioactivity ratios were 2.5 ± 0.9 and 2.9 ± 0.6 for HPAF-II/blood and BxPC-3/blood, respectively. Consistent biodistribution data were obtained in non-tumor-bearing Alcam−^/^− mice (n = 2) at 4 h after injection of ^64^Cu-DOTA-CysDb (Table 1), suggesting that accumulation of the probe in the liver and kidneys is not due to ALCAM expression.

Table 1. Biodistribution of 64Cu-DOTA-CysDb in mice bearing HPAF-II or BxPC-3 and C6 tumors and in Alcam-knockout mice

Tissue | Percent of ID/g (mean ± SD)
Tissue | HPAF-II (n = 5) | BxPC-3 (n = 4) | Alcam-knockout (n = 2)
Tissue | 21 h | 21 h | 4 h
Liver | 6.6 ± 0.5 | 6.8 ± 1.4 | 5.4 ± 0.1
Spleen | 1.7 ± 0.2 | 1.8 ± 0.3 | 2.2 ± 0.7
Kidneys | 42 ± 5.0 | 40 ± 0.8 | 90 ± 3.5
Lung | 1.8 ± 0.5 | 2.3 ± 0.3 | 2.1 ± 0.3
Blood | 0.7 ± 0.1 | 0.9 ± 0.1 | 1.0 ± 0.3
Positive tumor (T) | 1.8 ± 0.5 | 2.5 ± 0.5
Negative tumor (C6) | 1.0 ± 0.1 | 1.0 ± 0.1
T/blood | 2.5 ± 0.9 | 2.9 ± 0.6
T/C6 | 1.9 ± 0.6 | 2.4 ± 0.6

The radioactive uptake was also measured directly from the PET images acquired at 4 h and 21 h (1). Images were normalized to the activity of the injected dose and animal body weight. Total image units were converted into total activity using a conversion factor determined from a ^64^Cu phantom, and the activity was decay-corrected back to the time of dose calibration and injection to calculate the % ID/g for each region of interest. The uptake values in positive tumors at 21 h after injection were determined to be 1.6 ± 0.2% ID/g and 1.7 ± 0.4% ID/g for HPAF-II and BxPC-3, respectively. These values were lower than the corresponding ex vivo biodistribution values (P < 0.05), but the disparity was consistent. The uptake values at 4 h were slightly lower (P < 0.01), with 1.5 ± 0.2% ID/g for HPAF-II and 1.4 ± 0.5% ID/g for BxPC-3, but the tumor/background ratios (4.6 ± 1.1 and 5.1 ± 1.7 for HPAF-II at 4 h and 21 h, respectively; 5.4 ± 3.3 and 4.7 ± 3.2 for BxPC-3 at 4 h and 21 h, respectively) were not significantly different at the two time points (P > 0.5 for both HPAF-II and BxPC-3).

Immunohistochemistry of the harvested tumors confirmed that the HPAF-II and BxPC-3 tumors were positive for ALCAM, while the C6 tumors were negative, consistent with the results determined for each cell line in vitro (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term)]

No references are currently available.

## References

1 McCabe K.E., Liu B., Marks J.D., Tomlinson J.S., Wu H., Wu A.M. (2012). An engineered cysteine-modified diabody for imaging activated leukocyte cell adhesion molecule (ALCAM)-positive tumors. Mol Imaging Biol.
2 Olafsen T. (2010). andWu, A.M. Antibody vectors for imaging. Semin Nucl Med.
3 Kaur S., Venktaraman G., Jain M., Senapati S., Garg P.K., Batra S.K. (2012). Recent trends in antibody-based oncologic imaging. Cancer Lett.
4 Girgis M.D., Kenanova V., Olafsen T., McCabe K.E., Wu A.M., Tomlinson J.S. (2011). Anti-CA19-9 diabody as a PET imaging probe for pancreas cancer. J Surg Res.
5 Sirk S.J., Olafsen T., Barat B., Bauer K.B., Wu A.M. (2008). Site-specific, thiol-mediated conjugation of fluorescent probes to cysteine-modified diabodies targeting CD20 or HER2. Bioconjug Chem.
6 Shen B.Q., Xu K., Liu L., Raab H., Bhakta S., Kenrick M., Parsons-Reponte K.L., Tien J., Yu S.F., Mai E., Li D., Tibbitts J., Baudys J., Saad O.M., Scales S.J., McDonald P.J., Hass P.E., Eigenbrot C., Nguyen T., Solis W.A., Fuji R.N., Flagella K.M., Patel D., Spencer S.D., Khawli L.A., Ebens A., Wong W.L., Vandlen R., Kaur S., Sliwkowski M.X., Scheller R.H., Polakis P., Junutula J.R. (2012). Conjugation site modulates the in vivo stability and therapeutic activity of antibody-drug conjugates. Nat Biotechnol.
7 Vaidyanathan G. (1992). andZalutsky, M.R. Labeling proteins with fluorine-18 using N-succinimidyl 4-[18F]fluorobenzoate. Int J Rad Appl Instrum B.
8 Olafsen T., Sirk S.J., Olma S., Shen C.K., Wu A.M. (2012). ImmunoPET using engineered antibody fragments: fluorine-18 labeled diabodies for same-day imaging. Tumour Biol.